# Polyethylene glycol-Cys-Arg-Ser-Gly-Pro-Leu-Gly-Val-Tyr-[^18^F]fluorobenzoyl-Lys-Lys-tetramethylrhodamine

Chemical name: | Polyethylene glycol-Cys-Arg-Ser-Gly-Pro-Leu-Gly-Val-Tyr-[^18^F]fluorobenzoyl-Lys-Lys-tetramethylrhodamine
Abbreviated name: | PEG-peptide-[^18^F]-TMR
Synonym: | PEG-CRSGPLGVY-[^18^F]-KK-TMR
Agent category: | Peptide
Target: | Matrix metalloproteinases (MMPs)
Target category: | Enzyme
Method of detection: | Positron emission tomography (PET)
Source of signal/contrast: | ^18^F
Activation: | Yes
Studies: | - In vitro; - Rodents | No structure is currently available in PubChem (http://pubchem.ncbi.nlm.nih.gov/).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR)]

Extracellular matrix (ECM) adhesion molecules consist of a complex network of fibronectins, collagens, chondroitins, laminins, glycoproteins, heparin sulfate, tenascins, and proteoglycans that surround connective tissue cells, and they are mainly secreted by fibroblasts, chondroblasts, and osteoblasts (1). Cell substrate adhesion molecules are considered essential regulators of cell migration, differentiation, and tissue integrity and remodeling. These molecules play a role in inflammation and atherogenesis, but they also participate in the process of invasion and metastasis of malignant cells in the host tissue (2). Tumor cells adhere to the ECM, which provides a matrix environment for the permeation of tumor cells through the basal lamina and underlying interstitial stroma of the connective tissue. Overexpression of matrix metalloproteinases (MMPs) and other proteases by tumor cells allows intravasation of tumor cells into the circulatory system after degrading the basement membrane and ECM (3).

Several families of MMPs are involved in atherogenesis, myocardial infarction, angiogenesis, and tumor invasion and metastases (4-7). MMP expression is highly regulated in normal cells, such as trophoblasts, osteoclasts, neutrophils, and macrophages. Elevated levels of MMPs have been found in tumors associated with a poor prognosis for cancer patients (8). The peptide Gly-Pro-Leu-Gly-Val-Arg-NH_2_ (GPLGVR) was found to be a MMP2/9 substrate and is cleaved between the Gly (G) and Val (V) residues (9). Chuang et al. (10) linked a hydrophilic polyethylene glycol (PEG) group to the N-terminus of Cys-Arg-Ser-Gly-Pro-Leu-Gly-Val-Tyr-Lys-Lys (CRSGPLGVYKK) and a hydrophobic tetramethylrhodamine (TMR) molecule to the C-terminus Lys (K) residue to form PEG-CRSGPLGVYKK-TMR (PEG-peptide-TMR) for optical imaging of protease activity in vivo. Upon MMP cleavage, the lipophilic VYKK-TMR was released and accumulated at the sites (cell surface) of protease activity. The accumulation was most likely attributed to the binding of the lipophilic VYKK-TMR to the cell membrane non-specifically. For positron emission tomography (PET) imaging, the other Lys residue in PEG-peptide-TMR was labeled with 4-[^18^F]fluorobenzoate to form PEG-peptide-[^18^F]-TMR. PEG-peptide-[^18^F]-TMR accumulated in HT1080 tumors (with high MMP2 expression) but not in MCF-7 tumors (with low MMP2 expression), as determined with optical imaging in nude mice.

### Related Resource Links:

- Chapters in MICAD (MMP (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=books&Cmd=DetailsSearch&Term=matrix+metalloproteinases+AND+micad%5Bbook%5D))
- Gene information in NCBI (MMP2 (http://www.ncbi.nlm.nih.gov/gene/4313), MMP9 (http://www.ncbi.nlm.nih.gov/gene/4318))
- Articles in Online Mendelian Inheritance in Man (OMIM) (MMP2 (http://omim.org/entry/120360), MMP9 (http://omim.org/entry/120361))
- Clinical trials (MMP (http://www.clinicaltrials.gov/ct2/results?term=matrix+metalloproteinases))
- Drug information in FDA (MMP (http://google2.fda.gov/search?q=matrix+metalloproteinases+&client=FDAgov&site=FDAgov&lr=&proxystylesheet=FDAgov&output=xml_no_dtd&getfields=*&x=10&y=10))

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR)]

A solution of peptide-TMR (available commercially) and methoxy PEG_5000_-maleimide in phosphate-buffered saline (pH 7.4) was incubated for 4 h at room temperature (10). PEG-peptide-TMR was purified with column chromatography with 80%–90% purity. For ^18^F-labeling, a solution of N-succinimidyl-4-[^18^F]fluorobenzoate and PEG-peptide-TMR (370 nmol) was incubated for 30 min at 55°C. PEG-peptide-[^18^F]-TMR was isolated with high-performance liquid chromatography, with >95% radiochemical purity. The overall radiochemical yield of PEG-peptide-[^18^F]-TMR was 15% (based on H[^18^F]F), with a specific activity of 4 MBq/nmol (0.108 mCi/nmol) at the end of synthesis. The total synthesis time was not reported.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR%20and%20in%20vitro)]

Chuang et al. (10) showed that peptide-TMR (1.618 kDa) was cleaved by purified MMP2 and conditioned medium from MMP-expressing human fibrosarcoma HT1080 cells into two fragments: CRSGPLG (0.670 Da) and VYKK-TMR (0.948 kDa). The cleavage of peptide-TMR was inhibited by a broad-spectrum MMP inhibitor, 1,10-phenanthroline. Conditioned medium from human breast adenocarcinoma MCF-7 cells (with low MMP expression) was unable to cleave peptide-TMR. The reactions were monitored with matrix-assisted laser desorption/ionization-time-of-flight (MALDI-TOF). HT1080 cells or MCF-7 cells were incubated with 0.037 MBq (1 µCi) PEG-peptide-[^18^F]-TMR in the presence or absence of 1,10-phenanthroline (10 µM) for 1 h at 37°C and washed. The accumulated radioactivity levels in HT1080 and MCF-7 cells were 36,900 ± 8,700 cpm and 4,100 ± 550 cpm (P < 0.01), respectively. The 1,10-phenanthroline decreased the accumulation of radioactivity to 940 ± 300 cpm in HT1080 cells (P < 0.01). There was also some inhibition in the MCF-7 cells by 1,10-phenanthroline.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR%20and%20rodentia)]

Chuang et al. (10) performed ex vivo biodistribution studies of 3.7 MBq (0.1 mCi) PEG-peptide-[^18^F]-TMR in nude mice (n = 3/group) bearing HT1080 tumors (high MMP2 expression) and MCF-7 tumors (low MMP2 expression) in their right and left hind legs, respectively, at 15, 60, and 120 min after intravenous injection. The accumulation in HT1080 tumors was 6% injected dose/gram (ID/g), 11% ID/g, and 3% ID/g at 15, 60, and 120 min after injection, respectively. HT1080 tumors exhibited 4.3-, 18.4-, and 20.4-fold higher radioactivity than what was found in MCF-7 tumors at 15, 60, and 120 min after injection (P < 0.05). PEG-peptide-[^18^F]-TMR was cleared from the blood with an initial half-life (α) of 4.5 min and a terminal half-life (β) of 36.5 min. The organ with the highest accumulation was the kidney (9% ID/g) at 15 min, with 4% ID/g at 60 min and 1% at 120 min. The radioactivity retained in the kidneys was most likely due to the elimination of the tracer in urine. The other organs accumulated lesser radioactivity than the HT1080 tumors at these time points, and their radioactivity was cleared rapidly.

Whole-body PET imaging was performed in nude mice (n = 3/group) bearing HT1080 tumors in their right legs and MCF-7 tumors in their left hind legs at 15, 60, and 120 min after injection (10). In HT1080 tumors, good image intensity was visualized at 15 min, and the intensity reached a maximum at 60 min. On the other hand, little intensity was observed in MCF-7 tumors at these time points. HT1080 tumors exhibited 3.7-, 17.4-, and 18.4-fold higher radioactivity than what was found in MCF-7 tumors at 15, 60, and 120 min after injection, respectively. Pretreatment with 1,10-phenanthroline (20 mg/kg/d for 3 d) prior to the tracer injection reduced the radioactivity in HT1080 tumors to 1.3-, 3.6-, and 3.3-fold higher than what was found in MCF-7 tumors at 15, 60, and 120 min after injection, respectively.

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR%20and%20%28dog%20or%20pig%20or%20sheep%20or%20rabbit%29)]

No publication is currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR%20and%20%28primate%20not%20human%29)]

No publication is currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/entrez/query.fcgi?cmd=PureSearch&db=pubmed&details_term=MMP%20TMR%20and%20human)]

No publication is currently available.

## References

1 Bosman F.T., Stamenkovic I. (2003). Functional structure and composition of the extracellular matrix. J Pathol.
2 Jiang W.G., Puntis M.C., Hallett M.B. (1994). Molecular and cellular basis of cancer invasion and metastasis: implications for treatment. Br J Surg.
3 Albelda S.M. (1993). Role of integrins and other cell adhesion molecules in tumor progression and metastasis. Lab Invest.
4 Keppler D., Sameni M., Moin K., Mikkelsen T., Diglio C.A., Sloane B.F. (1996). Tumor progression and angiogenesis: cathepsin B & Co. Biochem Cell Biol.
5 Liu J., Sukhova G.K., Sun J.S., Xu W.H., Libby P., Shi G.P. (2004). Lysosomal cysteine proteases in atherosclerosis. Arterioscler Thromb Vasc Biol.
6 Berchem G., Glondu M., Gleizes M., Brouillet J.P., Vignon F., Garcia M., Liaudet-Coopman E. (2002). Cathepsin-D affects multiple tumor progression steps in vivo: proliferation, angiogenesis and apoptosis. Oncogene.
7 Brix, K., A. Dunkhorst, K. Mayer, and S. Jordans, Cysteine cathepsins: Cellular roadmap to different functions. Biochimie, 2007
8 Deryugina E.I., Quigley J.P. (2006). Matrix metalloproteinases and tumor metastasis. Cancer Metastasis Rev.
9 Bae M., Cho S., Song J., Lee G.Y., Kim K., Yang J., Cho K., Kim S.Y., Byun Y. (2003). Metalloprotease-specific poly(ethylene glycol) methyl ether-peptide-doxorubicin conjugate for targeting anticancer drug delivery based on angiogenesis. Drugs Exp Clin Res.
10 Chuang C.H., Chuang K.H., Wang H.E., Roffler S.R., Shiea J.T., Tzou S.C., Cheng T.C., Kao C.H., Wu S.Y., Tseng W.L., Cheng C.M., Hou M.F., Wang J.M., Cheng T.L. (2012). In Vivo Positron Emission Tomography Imaging of Protease Activity by Generation of a Hydrophobic Product from a Noninhibitory Protease Substrate. Clin Cancer Res.